# Hyperpolarized [^13^C]-2-hydroxyethylpropionate

Chemical name: | Hyperpolarized [^13^C]-2-hydroxyethylpropionate
Abbreviated name: | HP[^13^C]HEPP
Synonym: | ^13^C-CM, AH-110626
Agent category: | Small molecule
Target: | Other
Target category: | Other -metabolism
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | ^13^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=13C+ hydroxyethylpropionate + hyperpolarized)]

The signal of nuclear magnetic resonance (NMR) is proportional to the thermal equilibrium polarization of nuclear spins. As a function of magnetic field strength and temperature, the thermal equilibrium polarization is normally very low. For instance, the polarization level (the population difference) is 5 × 10^-6^ for ^1^H and 1 × 10^-6^ for ^13^C at 1.5 T and at body temperature. Because the thermal equilibrium polarization increases proportionally with the magnetic field strength, magnetic resonance imaging (MRI) systems at field strengths of 3–11.7 T have been developed. A totally different approach for increasing the polarization of spins is to create an artificial, non-equilibrium distribution of nuclear spins called the hyperpolarized state (1). In this state, the polarization of spins can be increased by a factor of ~10^5^ compared with that in the thermal equilibrium state. This approach has been used to hyperpolarize a wide range of organic substances containing ^13^C by either parahydrogen-induced polarization (PHIP) (2) or by dynamic nuclear polarization (DNP) (3). The produced ^13^C signal allows for practical medical and diagnostic imaging (4). The potential applications of hyperpolarized ^13^C imaging include vascular imaging, perfusion imaging, catheter tracking and visualization, interventional applications, and metabolic/molecular imaging (1).

The PHIP method increases the nuclear polarization by a chemical reaction of parahydrogen with a substrate containing double or triple bonds (5). In parahydrogen, the two hydrogen nuclei are oriented antiparallel. This is a non-equilibrium state in which the magnetic moments of the hydrogen nuclei cancel mutually (1). The parahydrogen molecule is added as a whole unit onto substrates by rhodium-catalyzed hydrogenation. Then the non-equilibrium spin polarization of parahydrogen is converted to the nuclear polarization of a vicinal ^13^C nucleus by diabatic-adiabatic magnetic field cycling (6, 7) or by radiofrequency (RF) pulses (8, 9). The magnetic field-cycling method involves two consecutive steps. The magnetic field is first suddenly dropped to nearly zero (<10 nT) from a high field value, followed by an adiabatic increase of the magnetic field up to 100 μT (7). By recycling the external magnetic field strength, the proton-carbon spins are brought into the strong coupling regime where the polarization is transferred from parahydrogen to carbon nuclei. The RF pulse sequence method uses the insensitive nuclei enhanced by polarization transfer (INEPT) mechanism to accomplish the polarization transfer between parahydrogen and ^13^C nuclei (8, 9). Currently, polarization levels of 20–30% can be obtained by the PHIP method for a substrate such as 2-hydroxyethylacrylate (1). Its hydrogenated product (2-hydroxyethylpropionate, abbreviated as HP[^13^C]HEPP) can be injected into subjects at a concentration range of 0.3 to 1.2 M in 2–3 ml. The injected HP[^13^C]HEPP can reach hearts and lungs in <10 s in rodents. An estimated concentration is in the range of 2 to 40 mM for the first pass. This provides a reasonable time window to collect signals in major organs and access changes in molecular structures of metabolic process.

A major difference between hyperpolarized ^13^C MRI and conventional MRI is that the magnetization of hyperpolarized ^13^C is created outside the MRI imager in a polarized system (10). Once the hyperpolarization has been created, the polarization will strive to return to the thermal equilibrium level at a rate governed by T_1_ relaxation time, which typically ranges from a few seconds to several minutes for ^13^C depending on the functional groups present. The corresponding time window for imaging is approximately a few minutes. Because 1.1% natural abundance of ^13^C produces negligible ^13^C signal, there is as a result virtually no background signal other than noise from the patient and the coil/receiver system. The injected HP[^13^C]HEPP generates a ^13^C signal that is linearly proportional to its concentration (10). In this respect, hyperpolarized ^13^C MRI behaves in a manner similar to modalities such as positron emission tomography (PET) and single-photon emission tomography (SPECT), where the signal amplitude is directly proportional to concentration of the agents. However, PET and SPECT have much higher sensitivities, allowing for detection of tracers at 10^-8^ M. The lack of background signal is advantageous in many applications such as angiography and perfusion, in which collection of additional proton images is required to provide anatomic interpretations. The small molecular size of HP[^13^C]HEPP qualifies it as an extracellular fluid (ECF) MRI contrast agent (10), suitable for pharmacokinetic tracing. HP[^13^C]HEPP remains mainly within the vascular bed during the first few circulations in the body. Subsequently, HP[^13^C]HEPP is distributed into the extracellular space and is finally excreted through the kidneys.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(13C+ hydroxyethylpropionate + hyperpolarized)+AND+synthesis%0D%0A)]

Goldman et al. detailed the procedure of generating HP[^13^C]HEPP (7). First, parahydrogen at ~97% purity was produced by passing hydrogen gas through a commercial catalyst (Ironex O-P catalyst or C*Chem) at a temperature of 14 K. A reactor chamber was pressurized with the parahydrogen to 10 bar and warmed to 60°C to speed the hydrogenation process. Next, ^13^C-labeled 2-hydroxyethylacrylate (molecular weight ~120 Da) and a rhodium catalyst were injected into the reaction chamber for hydrogenation to yield 2-hydroxyethylpropionate. For the field-cycling technique (7), the producing liquid was transferred into a low-field chamber of 10 μT and held for 0.5 s; then the field was decreased to 30 nT in 1 ms and subsequently increased exponentially back to 100 μT in 1 s. This polarized solution was filtered to remove the catalyst; a fraction of the solution was used for polarization calibration by NMR and the rest was transferred to a syringe for imaging purposes. The whole process was controlled by computer. For the RF pulse irradiation technique (9), the produced liquid was filtered and then subjected to an INEPT-type RF pulse sequence, which transferred the spin order from the parahydrogen on the hydrogenated molecules to the vicinal quaternary ^13^C nuclei. Both techniques provided a maximum ^13^C polarization at 20–30%, which was ~2 × 10^5^ times the thermal equilibrium value (7).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(13C+ hydroxyethylpropionate + hyperpolarized)+AND+%22in+vitro%22)]

The ^13^C relaxation times T_1_ and T_2_ of HP[^13^C]HEPP were 45–60 s and 5–6 s in vivo at body temperature, respectively (10).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(13C+ hydroxyethylpropionate + hyperpolarized) +AND++rodentia)]

The use of HP[^13^C]HEPP as tracer was demonstrated with magnetic resonance angiography in the neck and head in guinea pigs (7). A 3-ml aqueous solution containing 0.5 M HP[^13^C]HEPP was injected into the aortic arch through an arterial catheter in 2 s. The polarization of ^13^C was obtained with the magnetic field cycling method, and its value was ~24%. The ^13^C images of the head were produced by use of the true-fast imaging with steady-state precession (trueFISP) method on a 1.5-T imager, which exhibited a well-defined network of blood vessels when HP[^13^C]HEPP passed through the vasculatures.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

HP[^13^C]HEPP was used in the coronary angiography in five pigs (average weight = 31 ± 4 kg) during a cardiac interventional MRI procedure (10). A 5-ml aqueous solution containing 0.5 M HP[^13^C]HEPP was injected through a coronary artery. The polarization of ^13^C (~25–30%) was obtained by the magnetic field cycling method. The ^13^C images were collected on a 1.5-T imager with the use of a fully balanced steady-state free precession (bSSFP) pulse sequence. The coronary arteries were well depicted with signal/noise ratios of 10–40. HP[^13^C]HEPP was also used to perform real-time catheter tracking in pigs at 1.5 T (11). A 20% polarization of ^13^C was obtained by RF pulse irradiations to facilitate the polarization transfer from the proton nuclei to ^13^C nuclei. Under X-ray fluoroscopic guidance, a catheter over a guidewire was inserted into the left renal artery or the aortic arch. Coronal and sagittal ^13^C projection images of the catheter were acquired in an interleaved fashion while moving the catheter through the aortic arch of the pig. The entire length of the moving ^13^C catheter could be visualized in vivo using a standard bSSFP interleaved dual projection imaging protocol. The movement of catheter was visualized with a frame rate of one dual projection frame per 600–800 ms with typical signal/noise reduction ratios of 70–90.

The HP[^13^C]HEPP was used to image pulmonary vasculatures and parenchyma in pigs (9). High spatial and temporal resolution images of pulmonary perfusion were obtained at 1.5 T with this contrast technique. A partially deuterated HP[^13^C]HEPP (D-HP[^13^C]HEPP), which has a T_1_ relaxation time of 138 ± 8 s, longer than the 45 s in the non-deuterated analog, was used in the study. After injection of 5 ml of 0.3-M D-HP[^13^C]HEPP into the femoral vein in 5 s, the images displayed the time-dependent behavior of the injected D-HP[^13^C]HEPP, which flowed through the inferior vena cava and into the pulmonary arteries before being distributed throughout the lung parenchyma. HP[^13^C]HEPP was used to measure renal cortical blood flow in rabbits at 1.5 T (12). A 0.30-M HP[^13^C]HEPP solution with polarization of 25–30% was injected in 1 s via ear veins. The renal cortical blood flow was estimated to be 5.6 ± 1.4 ml/min per ml of kidney tissues, and the mean transit time in the renal arteries was determined to be 1.45 ± 0.07 s.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(13C+ hydroxyethylpropionate + hyperpolarized) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(13C+ hydroxyethylpropionate + hyperpolarized) +AND+human)]

No publication is currently available.

### NIH Support

HL 077241, RR002305

## References

1 Mansson S., Johansson E., Magnusson P., Chai C.M., Hansson G., Petersson J.S., Stahlberg F., Golman K. (2006). 13C imaging-a new diagnostic platform. Eur Radiol.
2 Bowers C.R., Weitekamp D.P. (1987). Parahydrogen and synthesis allow dramtically enhanced nuclear alignment. 109. J. Am. Chem. Soc.
3 Abragam, A., The principles of nuclear magnetisms. 1961
4 Golman K., Ardenkjaer-Larsen J.H., Petersson J.S., Mansson S., Leunbach I. (2003). Molecular imaging with endogenous substances. Proc Natl Acad Sci U S A.
5 Ardenkjaer-Larsen J.H., Fridlund B., Gram A., Hansson G., Hansson L., Lerche M.H., Servin R., Thaning M., Golman K. (2003). Increase in signal-to-noise ratio of > 10,000 times in liquid-state NMR. Proc Natl Acad Sci U S A.
6 Golman K., Axelsson O., Johannesson H., Mansson S., Olofsson C., Petersson J.S. (2001). Parahydrogen-induced polarization in imaging: subsecond (13)C angiography. Magn Reson Med.
7 Goldman M., Johannesson H., Axelsson O., Karlsson M. (2005). Hyperpolarization of 13C through order transfer from parahydrogen: a new contrast agent for MRI. Magn Reson Imaging.
8 Goldman M., Johannesson H. (2005). Conversion of a proton pair para order into 13C polarization by rf irradiation, for use in MRI. C. R. Physique.
9 Ishii M., Emami K., Kadlecek S., Petersson J.S., Golman K., Vahdat V., Yu J., Cadman R.V., MacDuffie-Woodburn J., Stephen M., Lipson D.A., Rizi R.R. (2007). Hyperpolarized 13C MRI of the pulmonary vasculature and parenchyma. Magn Reson Med.
10 Olsson L.E., Chai C.M., Axelsson O., Karlsson M., Golman K., Petersson J.S. (2006). MR coronary angiography in pigs with intraarterial injections of a hyperpolarized 13C substance. Magn Reson Med.
11 Magnusson P., Johansson E., Mansson S., Petersson J.S., Chai C.M., Hansson G., Axelsson O., Golman K. (2007). Passive catheter tracking during interventional MRI using hyperpolarized 13C. Magn Reson Med.
12 Johansson E., Olsson L.E., Mansson S., Petersson J.S., Golman K., Stahlberg F., Wirestam R. (2004). Perfusion assessment with bolus differentiation: a technique applicable to hyperpolarized tracers. Magn Reson Med.